# A15 (NIRF agent)

Chemical name: | A15
Abbreviated name: | A15
Synonym:
Agent Category: | Peptide
Target: | Activated coagulation factor XIIIa (FXIIIa)
Target Category: | Binding
Method of detection: | Optical imaging (NIRF)
Source of signal: | A15
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi)]

Thrombosis plays a major role in many cardiovascular diseases such as myocardial infarction, pulmonary embolism, deep venous thrombosis or cerebral venous thrombosis (CVT) (1). Unfortunately, the clinical diagnosis of CVT is complex, as most of its symptoms are non-specific and the well-established modalities such as conventional angiography, CT or MR venography, do not offer readily available information on chronicity or activity without serial anatomic testing over time (2).

Thrombosis occurs by an activation process of thrombin, which then converts fibrinogen into fibrin. Thrombin initiates the crosslinking of the polymerized fibrin via the activation of a transaminase called coagulation factor XIII (FXIIIa = activated factor XIII) (3). FXIIIa augments acute thrombus stability by rapidly crosslinking fibrin α- and γ-chains, and by covalently binding to alpha-2 antiplasmin (α2AP) (4) FXIIIa has a catalytic half-life of ~ 20 min, in vivo (5). Optical imaging with a FXIIIa probe may be a useful tool in the diagnostic of thrombosis (including CVT) and may provide valuable information currently unavailable through anatomically-based imaging modalities (6, 7).

A15 is a novel near-infrared fluorescence (NIRF) probe recognized by the enzyme FXIIIa and that covalently binds to fibrin by means of the transglutamase activity of FXIIIa. Preliminary research has shown that A15 is capable of testing the activity of FXIIIa and visualizing thrombus in vivo (8, 9). A15 may find applications as a molecular diagnostic tool for therapy with fibrinolytic or anti-FXIIIa agents, direct or indirect inhibitors, and other drugs for diseases such as CVT, ischemic stroke or myocardial infarction. Additional and more extensive research studies are needed to fully assess the potential and possible clinical benefits of the A15-NIRF imaging modality (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi)]

A15 can be prepared by solid-state peptide synthesis, as described by Tung et al. (10). Briefly, an acetyl glycine group is added to the N terminus of the α2AP fragment for capping, and a tryptophan residue and a cysteine residue are then added to the C terminus for quantitation and conjugation purposes. A15 is then labeled with a sulfhydryl reactive fluorochrome (Alexa Fluor 680C2 maleimide, AF680) via the C-terminal cysteine side chain (in sodium acetate buffer, at pH 6.5). After purification by HPLC, the final A15 product shows an excitation wavelength of 679 nM and an emission wavelength of 702 nm (9).

In addition to synthesizing A15, Tung et al. (10) and Jaffer et al (8). also prepared a control probe CA15 by replacing the glutamine residue at position 14 with an alanine residue. The fluorescent signal obtained with CA15 was less than 3 fold higher than the background signal, compared with a 11 fold enhancement for A15.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi%20AND%20in%20vitro)]

Tung et al. (10) performed in vitro assays using both A15 and CA15 probes (1µM) to assess the importance of the glutamine residue at position 14 in the crosslinking reaction with FXIII. The experimental protocol involved using mouse blood clots that were homogenized, washed in phosphate buffered saline and incubated with either A15 or CA15. Subsequent imaging of the clots (imaging system with a 630 + 15 nm excitation and a 700 + 20 nm emission) revealed the critical role of the glutamine residue. An intense fluorescence signal (fluorescence intensity ~ 760 AU, n = 3 clots tested) was obtained for the clot incubated with A15 (11 fold higher than the background of the blood), whereas a much weaker signal (fluorescence intensity ~ 200 AU, n = 3) for the clot incubated with the control probe CA15 (less than 3 fold higher than background).

Using human plasma clots, Jaffer et al. (8) investigated the ability of A15 to be crosslinked by human FXIIIa. The experimental protocol involved creating clots by mixing 90 µl of fresh frozen plasma with 3 µl of A15, CA15 (control probe), AF680 (free NIRF fluorochrome) or normal saline. All imaging agents were used at a concentration of 100 µmol/l, based on AF680. After incubation of the plasma clots with the individual imaging agents (90 min, 37°C), NIRF imaging was performed with each group (11). The collected data showed that in the A15 group, thrombi had a 347-fold NIRF signal increase compared with the saline (1562 ± 193.8 arbitrary units (AU) for A15 and 4.5 ± 0.6 AU for saline, P<0.001 A15 vs. each other group) and a 4.8 to 6.3-fold increase over the other control groups (247.5 ± 65.6 AU for CA15 and 328.0 ± 72.9 AU). Pre-incubation of FFP thrombi with IAA, a FXIII inhibitor, substantially reduced the A15 thrombus enhancement by 92.9% (P<0.001), supporting the fact that A15 is ‘FXIIIa-specific’.

The authors also showed that A15 was crosslinked to fibrin by FXIIIa, by performing a Western blot protein analysis (5) that used denaturated clots subjected to immunoblotting, and a polyclonal antibody that bound to the N-terminal peptide of the α_2_AP factor forming the backbone of A15. Clots formed with A15 (mass of A15 < 3kDa) showed a band at ~70 kDa that appeared strongly immunoreactive with the antibody to the N- terminus of α_2_AP. (No band was detected with CA15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi%20AND%20rodentia%5BMeSH%5D)]

Several studies aimed at assessing the ability of A15 to detect FXIII activity in vivo have been reported in the literature (8, 9, 12). One of them (8) was based on an intravascular model of thrombosis using 11 mice injected with A15 following the topical application of ferric chloride (FeCl_3_) onto femoral vessels exposed by blunt dissection. 6 mice received A15 (n = 3) or CA15 (n = 3), 30 min after application of FeCl_3_. 2 mice received A15 at either 0 or 120 min after application of FeCl_3,_ and 3 mice received A15 28 hours after application of FeCl_3_.

Fluorescence signals obtained for all animals having received the A15 showed a NIR enhancement characteristic of acute thrombi, with particular enhancements in the region of the femoral artery and vein within 30 to 45 min after application of FeCl_3_. In mice that received the imaging agent 30 min after application of FeCl_3_, the peak contrast -to-noise ratio between thrombus and background was 15.0 ± 6.7% by 90 min. In comparison, the value obtained for the mice having received the control probe CA15 was -1.4 ± 2.5% (P = 0.039). No thrombosis enhancement in the femoral vessels was observed in mice treated with A15, 28 h after application of FeCl_3_. This last result was found consistent with an expected decline in FXIIIa activity over time (5). Jaffer et al (8). suggested that crosslinking of A15 to fibrin might explain how thrombus contrast increased over time, and that higher contrast might be obtained in the absence of fibrinolysis (or embolization), for time periods occurring after 90 min post-application of FeCl_3._

In a study by Kim et al. (9), thrombi were formed in 12 CD-1 mice by application of paper strips (1 x 5 mm^2^) soaked in 10% FeCl_3_ onto the entire superior sagittal sinus (SSS) exposed by craniotomy (5 mm diameter). After an intravenous injection of A15 (5nmol/150 µl), light (exposure time = 1 sec) and serial fluorescence digital images (exposure time = 3 sec) were recorded at 0, 1, 3, 5, 10, 15, 20 and 25 min.

The following observations were made: the mice that had been exposed to FeCl_3_ only at the posterior 2.5 mm portion of the SSS exhibited a fluorescence signal limited to this same area. On the other hand, the animals whose entire 5 mm region had been exposed displayed a NIR signal in the entire SS and nearby branching vessels. The mean length of the SS showing the A15 signal appeared significantly longer in the full-length thrombosis group (2.8 ± 0.3) than in the localized thrombosis group (1.8 ± 0.5, P < 0.05). After intravenous injection, A15 first produced a cerebral angiogram, and was thereafter rapidly washed out in all but thrombosed areas, resulting in an improvement in target/background signal that allowed thrombosed areas to be identified by 5 to 10 min after injection of A15.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi%20AND%20%28dog%20OR%20rabbit%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi%20AND%20%28primates%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A15%20AND%20fluorescence%20AND%20thrombi%20AND%20human)]

No publication is currently available

## References

1 Corti R, Farkouh ME, Badimon JJ. (2002). The vulnerable plaque and acute coronary syndromes. Am J Med.
2 Sampson FC, Goodacre SW, Thomas SM, van Beek EJ. (2006). The accuracy of MRI in diagnosis of suspected deep vein thrombosis: systematic review and meta-analysis. Eur Radiol.
3 Bereczky Z, Katona E, Muszbek L. (2003). Fibrin stabilization (factor XIII), fibrin structure and thrombosis. Pathophysiol Haemost Thromb.
4 Muszbek L, Yee VC, Hevessy Z. (1999). Blood coagulation factor XIII: structure and function. Thromb Res.
5 Robinson BR, Houng AK, Reed GL. (2000). Catalytic life of activated factor XIII in thrombi. Implications for fibrinolytic resistance and thrombus aging. Circulation.
6 Renowden S. (2004). Cerebral venous sinus thrombosis. Eur Radiol.
7 Connor SE, Jarosz JM. (2002). Magnetic resonance imaging of cerebral venous sinus thrombosis. Clin Radiol.
8 Jaffer FA, Tung CH, Wykrzykowska JJ, Ho NH, Houng AK, Reed GL, Weissleder R. (2004). Molecular imaging of factor XIIIa activity in thrombosis using a novel, near-infrared fluorescent contrast agent that covalently links to thrombi. Circulation.
9 Kim DE, Schellingerhout D, Jaffer FA, Weissleder R, Tung CH. (2005). Near-infrared fluorescent imaging of cerebral thrombi and blood-brain barrier disruption in a mouse model of cerebral venous sinus thrombosis. J Cereb Blood Flow Metab.
10 Tung CH, Ho NH, Zeng Q, Tang Y, Jaffer FA, Reed GL, Weissleder R. (2003). Novel factor XIII probes for blood coagulation imaging. ChemBioChem.
11 Mahmood U, Tung CH, Bogdanov A, Weissleder R. (1999). Near-infrared optical imaging of protease activity for tumor detection. Radiology.
12 Jaffer FA, Tung CH, Gerszten RE, Weissleder R. (2002). In vivo imaging of thrombin activity in experimental thrombi with thrombin-sensitive near-infrared molecular probe. Arterioscler Thromb Vasc Biol.